# Ultrasmall superparamagnetic iron oxide-anti-CD20 monoclonal antibody

Chemical name: | Ultrasmall superparamagnetic iron oxide-anti-CD20 monoclonal antibody
Abbreviated name: | USPIO-anti-CD20 MAb
Synonym:
Agent Category: | Antibody
Target: | CD20 antigen
Target Category: | Antibody-antigen binding
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal /contrast: | Ultrasmall superparamagnetic iron oxide (USPIO)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=115968), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=29773) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=931) for more information about CD20.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=USPIO-anti-CD20+antibody&WebEnv=0ugZnII93XBk9N1-jZFsyYxyqh91qMFANvlb-k27eD2ecN4epu40NEcbsLS7HcjSzs-vsWZn8srHH%40D46A25376519D990_0026SID&WebEnvRq=1)]

Ultrasmall superparamagnetic iron oxide-anti-CD20 monoclonal antibody (USPIO-anti-CD20 MAb) is a molecular imaging agent developed for magnetic resonance imaging (MRI) of CD20 antigen-positive B cell lymphomas (1). The in vitro magnetic properties of USPIO are reported to be a T_1_ relaxivity (r_1_) of 21.6 (mmol/liter·sec)−^1^ and a T_2_ relaxivity (r_2_) of 44.1 (mmol/liter·sec)−^1^ at 37ºC and 0.47 tesla (T), where mmol/liter is the concentration of iron oxide (2).

Conventional, water-soluble, paramagnetic contrast agents are generally metal chelates with unpaired electrons, and they work by shortening both T_1_ and T_2_ relaxation times of surrounding water protons to produce a signal-enhancing effect (3, 4). They distribute in the extracellular fluid and do not cross the intact blood–brain barrier (3-5). Another approach is the development of water-insoluble SPIO nanoparticles that comprise iron oxides such as magnetite (Fe_3_O_4_), maghemite (γFe_2_O_3_), or other ferrites (6, 7). Ferromagnetic crystals are composed of magnetized domains the size of a micron. Superparamagnetism occurs when the size of the crystals is smaller than the ferromagnetic domain (~30 nm). SPIO agents typically consist of an iron oxide core and a hydrophilic coating (8). They have very high relaxivities (R_1_ and R_2_), and the significant capacity of these particles to increase the susceptibility effect of the measured spin–spin relaxation time (T_2_*) is especially useful in MRI. This large T_2_* effect is the result of the non-homogeneous distribution of these superparamagnetic particles, which accelerates the loss of phase coherence of the spins contributing to the MRI signal. Clinically, SPIO are predominantly used for their negative enhancement effect on T_2_- and T_2_*-weighted sequences. This class of MRI agents includes large oral SPIO (300–3500 nm) agents, standard SPIO (60–150 nm) agents, USPIO (10–40 nm) agents, monocrystalline iron oxide (10–30 nm) nanoparticle (MION) agents, and cross-linked iron oxide (CLIO) agents (a form of MION with a cross-linked dextran coating) (9). Both the size and the surface properties of SPIO particles affect their pharmacokinetics, organ distribution, and intracellular uptake (10). Biologically, SPIO particles are usually taken up by the reticuloendothelial system and phagocytic cells. USPIO particles are less prone to liver uptake and are small enough to migrate across the capillary wall of tumors (11). They also represent a useful MRI label for developing molecular probes to target specific markers (1).

The CD20 antigen (B1) is a 35-kDa, cell-surface nonglycosylated, hydrophobic phosphoprotein expressed on normal and malignant B cells, and it does not shed, modulate, or internalize (12-14). B1 is present on ~9% of the peripheral blood mononuclear cell fraction and >90% of B cells from blood and lymphoid organs. Lymphoma cells from >90% of patients with B cell non-Hodgkin’s lymphoma (NHL) express this antigen. Despite the presence of CD20 on normal B cells, it is a good tumor target for molecular targeting with antibodies for the management of NHL. Baio et al. (1) demonstrated the successful use of a commercially available USPIO-anti-CD20 MAb conjugate for MRI imaging in a murine xenotransplant model.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=USPIO-anti-CD20+antibody&WebEnv=028YAt62pIGB9ozqbHK_1hS4iKoHDCR0fqws6zVvHZ9ZRtJitBtLDAZdjtIaM9DqgLrHTgT51cksj%40D46A25376519D990_0026SID&WebEnvRq=1)]

Numerous chemical methods can be used to synthesize SPIO, and they are generally complex processes because of the colloidal nature of SPIO (6). The prototype of USPIO was developed by Weissleder et al. (2), and it was obtained through size fractionation of a heterogeneous iron oxide preparation with use of gel chromatography. Other processes have produced USPIO from solution, aerosol, or vapor (6, 15). After synthesis, a coating is required to prevent destabilization and agglomeration of the colloidal suspension. Many polymeric coating materials have been used, such as dextran, carboxymethylated dextran, carboxydetran, starch, polyethylene glycol, arabinogalactan, glycosaminoglycan, organic siloxane, and sulphonated syrenedivinylbenzene. The surface coating of USPIO allows chemical linkage of functional groups to couple macromolecules to nanoparticles. Oxidative and non-oxidative processes have been used to couple antibodies to USPIO (6). Baio et al. (1) used commercially available USPIO bound to an anti-CD20 MAb (IgG_1_-murine) stabilized with sodium citrate. The particles were composed of a biodegradable, nontoxic, ferromagnetic matrix (dextran). The overall mean particle diameter was ~30–50 nm. There were typically 10–200 antibody molecules/particle (30 nm in diameter). The in vitro R_1_ and R_2_ relaxivities measured at 37ºC and 1.5 T were 30 and 60 liter·s−^1^·mmol−^1^, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-anti-CD20%20antibody%20AND%20in%20vitro)]

Baio et al. (1) studied the in vitro binding of USPIO-anti-CD20 MAb to human D430B cells (anaplastic large-cell lymphoma B cell line) and Raji Burkitt lymphoma cells. After incubation with the USPIO-MAb conjugates, unbound conjugates were removed and cells were included in a matrigel sponge for MRI imaging with a 1.5-T MRI system. Immunofluorescence analysis showed that USPIO-anti-CD20 MAb bound to the cell surface, and the D4308 cells expressed five times more CD20 molecules than the Raji Burkitt cells. USPIO-anti-CD20 MAb on D430B cells showed a decrease in signal intensity (SI) on T_2_*-weighted images and SI enhancement on T_1_-weighted images. In comparison, USPIO-anti-CD20 MAb on Raji Burkitt cells only showed a slight hypointensity on T_2_-weighted images and a non-homogeneous hyperintensity on T_1_-weighted images. Quantitative analysis showed that the changes in T_1_ SI (ΔSI = SI_nonlableled_–SI _USPIO-anti-CD20 MAb_/noise) values from the three-dimensional fast-field echo sequences (3D-FFE) at 1.5 T for the USPIO-anti-CD20 MAb on D430B cells were −36.6, −12.4, and −6.2 for 0.03 μmol iron (Fe)/liter, 0.01 μmol Fe/liter, and 0.005 μmol Fe/liter USPIO-anti-CD20 MAb, respectively. The T_2_ ΔSI values were −73, −24, and −12 for 0.03 μmol Fe/liter, 0.01 μmol Fe/liter, and 0.005 μmol Fe/liter USPIO-anti-CD20 MAb, respectively. In comparison, the T_1_ ΔSI values of the USPIO-anti-CD20 MAb on Raji Burkitt cells were −25, −9, and −6 for 0.03 μmol Fe/liter, 0.01 μmol Fe/liter, and 0.005 μmol Fe/liter USPIO-anti-CD20 MAb, respectively. The T_2_ ΔSI values were −43, −17.7, and −12 for 0.03 μmol Fe/liter, 0.01 μmol Fe/liter, and 0.005 μmol Fe/liter USPIO-anti-CD20 MAb, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-anti-CD20%20antibody%20AND%20rodentia)]

MRI studies were performed in NOD-SCID mice bearing s.c. D430B or the Raji Burkitt tumors (0.5–1 cm^2^). Each mouse received an i.v. dose of 8 μmol Fe/kg 24 h before imaging with a 1.5 T-MRI system (1). The D430B tumors showed a non-homogeneous SI decrease on T_2_*-weighted images and a slight SI enhancement on T_1_-weighted images. In comparison, the Raji Burkitt tumors showed slight non-homogeneous hypointensity on T_2_*-weighted images and slight non-homogeneous hypertensity on T_1_-weighted images. Quantitative analysis studies were conducted with the region-of-interest technique to obtain the signal/noise (SNR) ratios. The T_2_*-weighted ΔSI value (SNR_before_/SNR_after_) of the D403B tumor (n = 5) was 35 ± 7% (82 ± 9%/57 ± 11%), whereas the T_2_*-weighted ΔSI value of the Raji Burkitt tumor was 15 ± 8% (47 ± 10%/40 ± 13%). In comparison, tumors in mice injected with a nonspecific standard SPIO agent ferumoxide (17 μmol Fe/kg) showed a T_2_*-weighted ΔSI value of 5 ± 6% (1,392 ± 86%/1,322 ± 80%). The authors concluded that 1.5 T-MRI could detect USPIO-antibody conjugates that target a tumor-associated antigen in vivo.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-anti-CD20%20antibody%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-anti-CD20%20antibody%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-anti-CD20%20antibody%20AND%20human)]

No publication is currently available.

## References

1 Baio G., Fabbi M., de Totero D., Ferrini S., Cilli M., Derchi L.E., Neumaier C.E. (2006). Magnetic resonance imaging at 1.5 T with immunospecific contrast agent in vitro and in vivo in a xenotransplant model. Magma.
2 Weissleder R., Elizondo G., Wittenberg J., Rabito C.A., Bengele H.H., Josephson L. (1990). Ultrasmall superparamagnetic iron oxide: characterization of a new class of contrast agents for MR imaging. Radiology.
3. Brasch, R.C., M.D. Ogan and B.L. Engelstad, Paramagnetic Contrast Agents and Their Application in NMR Imaging, in Contrast media; Biologic effects and clinical application, Z. Parvez, R., R. Monada and M. Sovak, Editor. 1987, CRC Press, Inc.: Boca Raton, Florida. p. 131-143.
4. Saini, S., J.T. Ferrucci, Enhanced Agents for Magnetic Resonance Imaging: Clinical Applications, in Pharmaceuticals in Medical Imaging, D.P. Swanson, H.M. Chilton and J.H. Thrall, Editor. 1990, MacMillan Publishing Co., Inc.: New York. p. 662-681.
5 Runge V.M., Kirsch J.E., Wells J.W., Awh M.H., Bittner D.F., Woolfolk C.E. (1993). Enhanced liver MR: Contrast agents and imaging strategy. Critical Reviews in Diagnostic Imaging.
6 Corot C., Robert P., Idee J.M., Port M. (2006). Recent advances in iron oxide nanocrystal technology for medical imaging. Adv Drug Deliv Rev.
7 Bulte J.W., Kraitchman D.L. (2004). Iron oxide MR contrast agents for molecular and cellular imaging. NMR Biomed.
8 Thorek D.L., Chen A.K., Czupryna J., Tsourkas A. (2006). Superparamagnetic iron oxide nanoparticle probes for molecular imaging. Ann Biomed Eng.
9 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
10 Fleige G., Seeberger F., Laux D., Kresse M., Taupitz M., Pilgrimm H., Zimmer C. (2002). In vitro characterization of two different ultrasmall iron oxide particles for magnetic resonance cell tracking. Invest Radiol.
11 Sun R., Dittrich J., Le-Huu M., Mueller M.M., Bedke J., Kartenbeck J., Lehmann W.D., Krueger R., Bock M., Huss R., Seliger C., Grone H.J., Misselwitz B., Semmler W., Kiessling F. (2005). Physical and biological characterization of superparamagnetic iron oxide- and ultrasmall superparamagnetic iron oxide-labeled cells: a comparison. Invest Radiol.
12 Hainsworth J.D. (2000). Monoclonal antibody therapy in lymphoid malignancies. Oncologist.
13 Tobinai K. (2003). Rituximab and other emerging antibodies as molecular target-based therapy of lymphoma. Int J Clin Oncol.
14 Zelenetz A.D. A clinical and scientific overview of tositumomab and iodine I 131 tositumomab Semin Oncol 2003 30Suppl 42 22 30 12728404
15 Gupta A.K., Gupta M. (2005). Synthesis and surface engineering of iron oxide nanoparticles for biomedical applications. Biomaterials.